# (Gd-chelate)_2_-Phe-His-Cys-Pro(OH)-Tyr(2-Cl)-Asp-Leu-Cys-His-Ile-Leu-(Gd-chelate)_2_

Chemical name: | (Gd-chelate)_2_-Phe-His-Cys-Pro(OH)-Tyr(2-Cl)-Asp-Leu-Cys-His-Ile-Leu-(Gd-chelate)_2_
Abbreviated name: | 4GdPeptide
Synonym: | EP-2104R (Gd-DOTA), EP-1873 (Gd-DTPA)
Agent category: | Peptide
Target: | Fibrin
Target category: | Acceptor
Method of detection: | Magnetic Resonance Imaging (MRI)
Source of signal/contrast: | Gadolinium
Activation: | No
Studies: | - In vitro; - Non-primate non-rodent mammals | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(EP-2104R))]

The acute formation of thrombus after atherosclerotic plaque rupture has been well recognized as the cause of unstable angina, myocardial infarction, transient ischemic attacks, and stroke (1, 2). Platelets and fibrin are the major components of all thrombi involved in the development and progression of atherosclerotic disease (3). MRI has shown promise in thrombus detection in both animals and humans (4), such as direct thrombus imaging based on the T_1_-shortening properties of endogenous methemogobin in venous thrombi (5) and enhancing the contrast between the myocardium and intracardiac by conventional gadolinium chelates (6). However, thrombosis is a dynamic process in which the thrombus material of different ages forms a layered structure due to successive mural deposition (7). MR signal of thrombi is complicated by the presence of platelets, fibrin, and red blood cells in the clots (7). Accurate thrombus age definition and detection of old and organized thrombi remain difficult. Since fibrin is abundant in all types of thrombi, including arterial, venous, acute, and chronic, fibrin-targeted contrast agents can be used to differentiate between layers of fibrin deposits in all types of thrombi and in superimposed thrombosis associated with plaque (3). The low concentration of fibrin present in plasma minimizes spurious background imaging signal (3).

Fibrin is formed after thrombin cleavage of fibrinopeptide A from fibrinogen Aα-chains, followed by polymerization and cross-linkage to form thick fibrin bundles and complex branched clot network (8). 4GdPeptide is a gadolinium based contrast agent designed to bind to fibrin (7). 4GdPeptide comprises a small peptide of 11 amino acids and two gadolinium chelates such as gadolinium-diethylenetriaminepentaacetic acid (Gd-DTPA) or gadolinium-1,4,7,10-tetraazcyclododecane-N,N’,N”,N”’-tetraacetate (Gd-DOTA) attached to each terminal (7, 9). Gd-DOTA has an in vitro stability five orders of magnitude greater than that of Gd-DTPA (10). This greater stability reduces the in vivo toxicity caused by the dissociation of free Gd(III) in the metabolic process (10). The small peptide contains one intramolecular disulfur bond, and binds to fibrin selectively and reversibly (9, 11). The binding to fibrin generates a field dependent paramagnetic enhancement effect (PRE) due to the increase of the effective rotation correlation time τ_R_ (12). No interactions and competitive binding with other proteins such as fibrinogen or collagen have been noted in both in vitro or in vivo (11). 4GdPeptide can penetrate through thrombi to bind fibrin in depth via passive diffusion; and distinguish between occlusive and non-occlusive arterial thrombi or between thrombi of different sizes and ages (11). Early-phase clinical studies (phase I and II) are currently testing the safety of 4GdPeptide in humans (11).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(EP-2104R)+AND+synthesis%0D%0A)]

Bontar et al. reported a detailed synthesis of the cyclic disulfide precursor of EP-2104R/EP-1873 (7). Phe-His-Cys-Pro(OH)-Tyr(3-Cl)-Asp-Leu-Cys-His-Ile-Leu (FHCP(OH)Y(3-Cl)DLCHIL), was prepared with the use of a diaminotryl resin, Fmoc coupling strategy, and thallium trifluoroacetate cyclization. Conjugation of 4 back-bone substituted Gd-DTPA or Gd-DOTA was achieved with the use of standard amide coupling chemistry, acid deprotection and subsequent complexation with GdCl_3_. There were four gadolinium chelates per peptide. The agent with chelates GD-DTPA was named as EP-1873 and that with chelates Gd-DOTA was EP-2104R. Both are commercially available (EPIX Medical Inc, MA).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(EP-2104R)+AND+%22in+vitro%22)]

The relaxation efficacy of EP-1873, the agent with Gd-DTPA moieties, was measured at 1.4T and 37 °C (7). The value of T_1_ relaxivity was 12 and 21 mM Gd^-1^ s^-1^ in buffer and fibrin, respectively. The binding of EP-1873 to fibrin was evaluated in Tris-buffered saline (7). K_d_ was determined to be 3.5 ±0.15 μmol/L for rabbit fibrin and 2.2 ±0.3 μmol/L for human fibrin. The number of binding sites was 2.4 in rabbit fibrins and 1.8 in human fibrin. In comparison, the binding constant for soluble fibrinogen was >200 μmol/L. EP-2104R remained within the thrombus for 1.5 to 2 hr due to its high binding affinity for fibrin and apparent slow excretion kinetics relative to its blood clearance (11). No interactions and competitive binding with other proteins such as fibrinogen or collagen were reported for both in vitro and in vivo experiments.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(EP-2104R) +AND++rodentia)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

The specificity of EP-1873 binding for fibrin was examined in a rabbit carotid artery/jugular vein stasis model (7). After co-injection of 2 μmol/kg ^153^Gd-labeled EP-1873 and 2 μmol/kg ^111^In-labled-Gd-DTPA, the uptake of ^153^Gd-labeled EP-1873 (88±36 μmol/L) in carotid thrombus or jugular thrombi was significantly higher than that of ^111^In-labeled Gd-DTPA (2.5±0.5 μmol/L). At 60 min post injection, the blood level was found to be 22±8 μmol/L for ^153^Gd-labeled EP-1873 and 5.6±1.5 μmol/L for ^111^In-labeled Gd-DTPA. The mean residence time of EP-1873 in plasma was 47±10 min.

The use of EP-1873 to detect acute and subacute thrombosis was conducted in rabbits (7). Thrombus was induced on injured abdominal aortic walls and activated by pharmacological trigger after 8-week high-cholesterol diet. After bolus injection of 2 μmol/kg EP-1873, Images were collected at a 1.5 T imager. The signal intensity exhibited persistent increase in the acute thrombi. This led to a contrast to noise ratio (CNR) of 12±7 between the thrombus and blood one hour after injection and 24±10 twenty hours later, yielding an average signal to noise ratio (SNR) of 18±8 and 28±10 for the thrombus. In comparison, the average SNR for the arterial blood was 4.5±1.2 and 4.2±1.2. The subacute thrombus was examined 1-3 days after plaque rupture, for which the corresponding CNR was 8±2 one hour after injection and 19±7 twenty hours later. The detection of chronic thrombus was demonstrated in rabbits by using EP-2104R (11), the agent with Gd-DOTA moieties. Arterial thrombosis was induced by carotid artery crush injury and blood stasis. The injured artery and the contralateral normal carotid artery were imaged at 5 μmol/kg dose shortly after thrombus induction. The images were also collected later as the thrombus advanced to different phases, including acute, subacute and chronic thrombus. EP-2104R can accurately detect occlusive and non-occlusive thrombi, regardless of their location, size, and organization stage.

The enhancement efficacy of EP-2104R was examined in the images of various thrombi in swine, including arterial thrombus (13), vein thrombus (14), pulmonary emboli (9, 15, 16), coronary thrombosis (15, 17) and atrial clots (18). In a coronary in-stent thrombosis model (13), all thrombi were observed after bolus injection of 60 μmol EP-2104R. The enhancement effect resulted in an average thrombus SNR and CNR of 11±2 and 9±2. Chemical analysis indicated that gadolinium concentration was 0.099 mM in a 38 mg thrombus and 0.147 mM in a 51 mg thrombus. In a cerebral sinus vein thrombosis model (14), acute thrombi formed in the superior sagittal sinus showed significant signal increase after bolus injection of 4 μmol/kg dose, allowing for discrimination between thrombus, blood pool and brain tissue. Gadolinium concentration in the thrombi ranged from 0.2 to 0.65 mM. The enhancement efficacy of EP-2104R in the clots made ex vivo was compared with that in the clots removed from patients (9, 17). In a pulmonary embolism (9), CNR was found to be 13±3 for the ex vivo engineered clots and 22±9 for the patient clots. Gadolinium concentration in the thrombi was determined to be 0.082±0.043 mM for the engineered clots and 0.247±0.044 mM for the patient clots respectively. Similar results were also found in a coronary arterial thrombosis in swine (17).

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(EP-2104R) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(EP-2104R) +AND+human)]

No details were currently available.

### NIH Support

HL71021, HL78667, HL61825

## References

1 Libby P. (2001). Current concepts of the pathogenesis of the acute coronary syndromes. Circulation.
2 Briley-Saebo K.C., Mulder W.J., Mani V., Hyafil F., Amirbekian V., Aguinaldo J.G., Fisher E.A., Fayad Z.A. (2007). Magnetic resonance imaging of vulnerable atherosclerotic plaques: current imaging strategies and molecular imaging probes. J Magn Reson Imaging.
3 Sirol M., Aguinaldo J.G., Graham P.B., Weisskoff R., Lauffer R., Mizsei G., Chereshnev I., Fallon J.T., Reis E., Fuster V., Toussaint J.F., Fayad Z.A. (2005). Fibrin-targeted contrast agent for improvement of in vivo acute thrombus detection with magnetic resonance imaging. Atherosclerosis.
4 Yuan C., Kerwin W.S., Yarnykh V.L., Cai J., Saam T., Chu B., Takaya N., Ferguson M.S., Underhill H., Xu D., Liu F., Hatsukami T.S. (2006). MRI of atherosclerosis in clinical trials. NMR Biomed.
5 Viereck J., Ruberg F.L., Qiao Y., Perez A.S., Detwiller K., Johnstone M., Hamilton J.A. (2005). MRI of atherothrombosis associated with plaque rupture. Arterioscler Thromb Vasc Biol.
6 Ala-Korpela M., Sipola P., Kaski K. (2006). Characterization and molecular detection of atherothrombosis by magnetic resonance--potential tools for individual risk assessment and diagnostics. Ann Med.
7 Botnar R.M., Perez A.S., Witte S., Wiethoff A.J., Laredo J., Hamilton J., Quist W., Parsons E.C., Vaidya A., Kolodziej A., Barrett J.A., Graham P.B., Weisskoff R.M., Manning W.J., Johnstone M.T. (2004). In vivo molecular imaging of acute and subacute thrombosis using a fibrin-binding magnetic resonance imaging contrast agent. Circulation.
8 Mosesson M.W. (2005). Fibrinogen and fibrin structure and functions. J Thromb Haemost.
9 Spuentrup E., Katoh M., Buecker A., Fausten B., Wiethoff A.J., Wildberger J.E., Haage P., Parsons E.C., Botnar R.M., Graham P.B., Vettelschoss M., Gunther R.W. (2007). Molecular MR imaging of human thrombi in a swine model of pulmonary embolism using a fibrin-specific contrast agent. Invest Radiol.
10 Bousquet J.C., Saini S., Stark D.D., Hahn P.F., Nigam M., Wittenberg J., Ferrucci J.T. (1988). Gd-DOTA: characterization of a new paramagnetic complex. Radiology.
11 Sirol M., Fuster V., Badimon J.J., Fallon J.T., Moreno P.R., Toussaint J.F., Fayad Z.A. (2005). Chronic thrombus detection with in vivo magnetic resonance imaging and a fibrin-targeted contrast agent. Circulation.
12 Lauffer R.B. (1987). Paramagnetic metal complexes as water proton relaxation agents for NMR imaging:Theory and design. Chem. Rev.
13 Botnar R.M., Buecker A., Wiethoff A.J., Parsons E.C., Katoh M., Katsimaglis G., Weisskoff R.M., Lauffer R.B., Graham P.B., Gunther R.W., Manning W.J., Spuentrup E. (2004). In vivo magnetic resonance imaging of coronary thrombosis using a fibrin-binding molecular magnetic resonance contrast agent. Circulation.
14 Stracke C.P., Katoh M., Wiethoff A.J., Parsons E.C., Spangenberg P., Spuntrup E. (2007). Molecular MRI of cerebral venous sinus thrombosis using a new fibrin-specific MR contrast agent. Stroke.
15 Spuentrup E., Buecker A., Katoh M., Wiethoff A.J., Parsons E.C., Botnar R.M., Weisskoff R.M., Graham P.B., Manning W.J., Gunther R.W. (2005). Molecular magnetic resonance imaging of coronary thrombosis and pulmonary emboli with a novel fibrin-targeted contrast agent. Circulation.
16 Spuentrup E., Katoh M., Wiethoff A.J., Parsons E.C., Botnar R.M., Mahnken A.H., Gunther R.W., Buecker A. (2005). Molecular magnetic resonance imaging of pulmonary emboli with a fibrin-specific contrast agent. Am J Respir Crit Care Med.
17 Spuentrup E., Katoh M., Wiethoff A.J., Buecker A., Botnar R.M., Parsons E.C., Guenther R.W. (2007). Molecular Coronary MR Imaging of Human Thrombi using EP-2104R, a Fibrin-Targeted Contrast Agent: Experimental Study in a Swine Model. Rofo.
18 Spuentrup E., Fausten B., Kinzel S., Wiethoff A.J., Botnar R.M., Graham P.B., Haller S., Katoh M., Parsons E.C., Manning W.J., Busch T., Gunther R.W., Buecker A. (2005). Molecular magnetic resonance imaging of atrial clots in a swine model. Circulation.